# ^99m^Tc-Hydrazinonicotinamide-epidermal growth factor

Chemical name: | ^99m^Tc-Hydrazinonicotinamide-epidermal growth factor
Abbreviated name: | ^99m^Tc-HYNIC-EGF
Synonym:
Agent category: | Polypeptide
Target: | Epidermal growth factor receptor (EGFR)
Target category: | Receptor
Method of detection: | Single photon emission computed tomography (SPECT)
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=41327732), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about EGFR.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc%5BAll%20Fields%5D%20AND%20EGF%5BAll%20Fields%5D)]

Epidermal growth factor (EGF) is a 53-amino acid cytokine (6.2 kDa) secreted by ectodermic cells, monocytes, kidneys and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF receptor (EGFR) is a transmembrane protein with an intracellular tyrosine kinase present on most cells. EGFR is overexpressed on many solid tumor cells, such as those of breast, non-small-cell lung, head and neck, and colon cancers (2-4). The high level of EGFR expression on cancer cells is associated with a poor prognosis (5-7). EGF has been labeled with ^99m^Tc by various laboratories as a potential SPECT imaging agent for EGFR expression on cancer cells (8-11).

The Ras protein is a key regulator in the signaling pathway of the EGFR. Inhibition of farnesylation of Ras in cancer cells by farnesyltransferase inhibitors (FTI) led to inhibition of tumor growth, up regulation of EGFR, and decreased internalization of EGFR (12). ^99m^Tc-HYNIC-EGF was developed for in vivo prediction of cancer cell response to FTI (8).

### Related Resource Links:

- Chapters in MICAD (EGFR (http://www.ncbi.nlm.nih.gov/books?term=EGFR%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (EGF (http://www.ncbi.nlm.nih.gov/gene/1950), EGFR (http://www.ncbi.nlm.nih.gov/gene/1956)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (EGF (http://www.ncbi.nlm.nih.gov/omim/131530), EGFR (http://www.ncbi.nlm.nih.gov/omim/131550))
- Clinical trials (EGF (http://www.clinicaltrials.gov/ct2/results?term=EGF))
- Drug information in FDA (EGF (http://google2.fda.gov/search?q=EGF&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=6&y=9))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc%20AND%20EGF%20AND%20synthesis)]

Hydrazinonicotinamide (HYNIC) was conjugated to human EGF to form HYNIC-EGF, which was purified by dialysis with a yield of >94% (8). A mixture of HYNIC-EGF and [^99m^Tc]pertechnetate (74–370 MBq, 2–10 mCi) in reaction solution was incubated at room temperature for 20 min. ^99m^Tc-HYNIC-EGF was purified by column chromatography to yield 81-95%, with a radiochemical purity of >95%. The specific activity of ^99m^Tc-HYNIC-EGF was 1.23 Bq/nmol (33 pCi/nmol) for in vitro binding studies and 3.7–7.4 MBq/nmol (0.1–0.2 mCi/nmol) for the biodistribution studies.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc%20AND%20EGF%20AND%20in%20vitro)]

^99m^Tc-HYNIC-EGF was found to be stable in Ham’s F12 cell growth medium at 25ºC up to 4 h (8). LoVo human colon adenocarcinoma cells showed a K_d_ of 3.6 nM with ^99m^Tc-HYNIC-EGF and 4.0 nM with [^125^I]EGF in saturation binding studies (8, 13). MAb88910 is a monoclonal antibody that inhibits EGF binding to EGFR. MAb88910 showed a K_i_ value of 1.7 nM and 1.3 nM for blocking ^99m^Tc-HYNIC-EGF and [^125^I]EGF binding to LoVo cells, respectively (8, 13).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc%20HYNIC%5BAll%20Fields%5D%20AND%20EGF%20and%20rodentia)]

Normal mice were injected with injected i.v. with ^99m^Tc-HYNIC-EGF (0.555 MBq, 0.015 mCi, 1 μg or 0.15 nmol) (8). The liver (55.0 ± 11.2% injected dose (ID)/g at 40 min) and kidneys (31.9 ± 18.4% ID/g at 5 min) were the major organs of uptake. A small amount was taken up by the small intestine (4.3 ± 1.8% ID/g at 2 h) and large intestine (7.7 ± 1.9% ID/g at 6 h) at later time points. Stomach activity was significantly higher than blood, beginning 20 min after injection. There was also some uptake in the spleen, which is maximal at 10 min after injection. After 48 h, only 52% of the injected ^99m^Tc-HYNIC-EGF was excreted, whereas the remaining radioactivity was in the liver, kidneys, and spleen.

^99m^Tc-HYNIC-hEGF was taken up in LoVo tumor tissue in tumor-bearing athymic mice (8). The tumor-to-thigh ratio was maximal at 2 h (2.5 ± 0.8). The nominal value of the uptake at 2 h was 3.5 ± 1.2%ID/g. Blocking with MAb88910 resulted in a decrease of the ratio from 2.5±0.8 to 1.2±0.2 (p<0.01). Co-injection of 100 μg of unlabelled EGF decreased the ratio to 1.1 ± 0.3 (p<0.01). In both cases, the muscle uptake did not change significantly. When comparing ^99m^Tc-HYNIC-EGF tumor uptake data to ^123^I-EGF values, no significant differences were seen. Both tracers showed a maximum tumor-to-thigh ratio at 2 h (^123^I-EGF uptake ratio at 2 h was 2.0 ± 0.3). Pretreatment of tumor-bearing mice with FTI inhibitor (R115777, 100 mg/kg) for 6-8 h before ^99m^Tc-HYNIC-EGF injection decreased the tumor-to-muscle ratio from 2.5 to 1.0. Similar results were also obtained using planar gamma scintigraphy imaging. The control experiment using ^99m^Tc-HSA showed that the effect of FTI inhibition was not due to an influence on vascularization (13).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc%20HYNIC%5BAll%20Fields%5D%20AND%20EGF%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc%20HYNIC%20AND%20EGF%20and%20%28primates%20not%20humans%29)]

No publication is currently available

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc%20HYNIC%20AND%20EGF%20and%20humans)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
3 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
4 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
5 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
6 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
7 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
8 Cornelissen B., Kersemans V., Burvenich I., Oltenfreiter R., Vanderheyden J.L., Boerman O., Vandewiele C., Slegers G. (2005). Synthesis, biodistribution and effects of farnesyltransferase inhibitor therapy on tumour uptake in mice of 99mTc labelled epidermal growth factor. Nucl Med Commun.
9 Rusckowski M., Qu T., Chang F., Hnatowich D.J. (1997). Technetium-99m labeled epidermal growth factor-tumor imaging in mice. J Pept Res.
10 Yang W., Barth R.F., Leveille R., Adams D.M., Ciesielski M., Fenstermaker R.A., Capala J. (2001). Evaluation of systemically administered radiolabeled epidermal growth factor as a brain tumor targeting agent. J Neurooncol.
11 Capala J., Barth R.F., Bailey M.Q., Fenstermaker R.A., Marek M.J., Rhodes B.A. (1997). Radiolabeling of epidermal growth factor with 99mTc and in vivo localization following intracerebral injection into normal and glioma-bearing rats. Bioconjug Chem.
12 End D.W., Smets G., Todd A.V., Applegate T.L., Fuery C.J., Angibaud P., Venet M., Sanz G., Poignet H., Skrzat S., Devine A., Wouters W., Bowden C. (2001). Characterization of the antitumor effects of the selective farnesyl protein transferase inhibitor R115777 in vivo and in vitro. Cancer Res.
13 Cornelissen B., Thonissen T., Kersemans V., Van De Wiele C., Lahorte C., Dierckx R.A., Slegers G. (2004). Influence of farnesyl transferase inhibitor treatment on epidermal growth factor receptor status. Nucl Med Biol.